# Anti-ligand–induced binding sites (LIBS) antibody conjugated to microparticles of iron oxide

Chemical name: | Anti-ligand–induced binding sites (LIBS) antibody conjugated to microparticles of iron oxide
Abbreviated name: | LIBS-MPIOs
Synonym:
Agent category: | Antibody, single-chain
Target: | Platelet glycoprotein GPIIb/IIIa receptor (CD61/CD41)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MPIO)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to increased contrast images.

Thrombosis plays a major role in many cardiovascular diseases, such as myocardial infarction, pulmonary embolism (PE), deep venous thrombosis (DVT), atherothrombosis, or cerebral venous thrombosis (2, 3). DVT is a significant cause of PE, which is a potentially life-threatening clinical problem. Thrombosis occurs when platelets deposit in regions of low flow in the deep venous system, followed by an activation process of thrombin, which then converts fibrinogen into fibrin. Platelets become activated and bind to fibrinogen, resulting in platelet aggregation via the platelet integrin GPIIb/IIIa (α_IIb_β_3_, CD61/CD41). The thrombus may become organized or detached from the vessel wall. A single-chain antibody (anti-LIBS 145) has been developed to recognize ligand-induced binding sites (LIBS) of GPIIb/IIIa that become exposed only upon receptor-ligand binding (4). Anti-LIBS 145 single-chain antibody does not bind to circulating platelets. Anti-LIBS 145 single-chain antibody was conjugated to microparticles of iron oxide (MPIOs) to form LIBS-MPIOs for T2-weighted MRI imaging of platelet-containing thrombi (5-8).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=GPIIb/IIIa%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/gene/3690), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/gene/3674))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=VCAM-1) (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=173470), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=607759))
- Clinical trials (Integrin (http://www.clinicaltrials.gov/ct2/results?term=integrin))
- Drug information in FDA (http://google2.fda.gov/search?q=integrin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=17&y=16)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MPIO+and+synthesis)]

Cobalt-functionalized MPIOs (1 mg, 1 µm in diameter) were incubated with LIBS containing histidine tag for 10 min at room temperature (8). LIBS-MPIOs were isolated with magnetic separation and washings. Approximately 10 µg LIBS antibody was conjugated to 1 mg MPIOs. An irrelevant single-chain control antibody was also conjugated to MPIOs. LIBS-MPIOs exhibited r_1_ and r_2_ relaxivity values of 0.05 ± 0.01 and 121.2 ± 6.8 mM^-1^s^-1^ (8), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MPIO+and+in+vitro)]

Confocal microscopy of human platelets immobilized on fibrinogen showed that LIBS-MPIOs bound to platelets co-localizing with anti-CD61 antibody (5). MPIOs conjugated with control antibody showed little binding to the platelets.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MPIO+and+rodentia)]

von zur Muhlen et al. (5) performed ex vivo T2-weighted MRI (11.7 T) of injured arterial segments perfused with 6.5 mg iron/kg LIBS-MPIOs (n = 7) or control MPIOs (n = 6). MRI signal decreases in the thrombosed artery were 23.7 and 6.2 for LIBS-MPIOs and control MPIOs (P < 0.01), respectively. There was a significantly higher binding (P < 0.01) for LIBS-MPIOs (9.98 LIBS-MPIOs/section) than control MPIOs (0.5 control MPIOs/section). Immunostaining with anti-CD61 confirmed the co-localization of LIBS-MPIOs and platelets adherent to the thrombosed arterial wall. An ex vivo biodistribution study was performed in mice (n = 3) at 0.5 h and 24 h after intravenous injection of 4.5 mg iron/kg. At 30 min, there were 7, 2, 32, and 110 LIBS-MPIOs/section for the kidney, lung, liver, and spleen, respectively. At 24 h, there were 2, 12, 28, and 100 LIBS-MPIOs/section for the kidney, lung, liver, and spleen, respectively. The high uptake in the liver and spleen represented sequestration of the nanoparticles by the phagocytes present in these organs. No blocking experiment was performed.

von zur Muhlen et al. (8) performed in vivo MRI (9.4 T) of thrombosis and thrombolysis in mice (n = 6–8 mice/group) exposed to 6% ferric chloride solution to injure the carotid artery. A significant signal decrease in the thrombosed artery was observed with LIBS-MPIOs but not with control MPIOs at 36 min after injection (P < 0.05). At 48 min after injection of LIBS-MPIOs, human or murine urokinase was injected to induce thrombolysis. Both urokinases reduced the signal decreases at 24–36 min after injection (P < 0.05). Histological examination of the arterial wall showed that there were 30, 3, and 4 LIBS-MPIOs/thrombus section for untreated, human urokinase-treated, and murine urokinase-treated mice. There was a significant correlation of the MPIO content with MRI signal voids (P < 0.01).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MPIO+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MPIO+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MPIO+and+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Corti R., Fuster V. (2003). New understanding, diagnosis, and prognosis of atherothrombosis and the role of imaging. Am J Cardiol.
3 Taillefer R. (2001). Radiolabeled peptides in the detection of deep venous thrombosis. Semin Nucl Med.
4 Schwarz M., Katagiri Y., Kotani M., Bassler N., Loeffler C., Bode C., Peter K. (2004). Reversibility versus persistence of GPIIb/IIIa blocker-induced conformational change of GPIIb/IIIa (alphaIIbbeta3, CD41/CD61). J Pharmacol Exp Ther.
5 von zur Muhlen C., Peter K., Ali Z.A., Schneider J.E., McAteer M.A., Neubauer S., Channon K.M., Bode C., Choudhury R.P. (2009). Visualization of activated platelets by targeted magnetic resonance imaging utilizing conformation-specific antibodies against glycoprotein IIb/IIIa. J Vasc Res.
6 von Zur Muhlen C., Sibson N.R., Peter K., Campbell S.J., Wilainam P., Grau G.E., Bode C., Choudhury R.P., Anthony D.C. (2008). A contrast agent recognizing activated platelets reveals murine cerebral malaria pathology undetectable by conventional MRI. J Clin Invest.
7 von Zur Muhlen C., von Elverfeldt D., Choudhury R.P., Ender J., Ahrens I., Schwarz M., Hennig J., Bode C., Peter K. (2008). Functionalized magnetic resonance contrast agent selectively binds to glycoprotein IIb/IIIa on activated human platelets under flow conditions and is detectable at clinically relevant field strengths. Mol Imaging.
8 von zur Muhlen C., von Elverfeldt D., Moeller J.A., Choudhury R.P., Paul D., Hagemeyer C.E., Olschewski M., Becker A., Neudorfer I., Bassler N., Schwarz M., Bode C., Peter K. (2008). Magnetic resonance imaging contrast agent targeted toward activated platelets allows in vivo detection of thrombosis and monitoring of thrombolysis. Circulation.